# ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-c(RGDyK)-Glu-6-aminohexanoic acid-bombesin[7-14]NH_2_

Chemical name: | ^64^Cu-1,4,7-Triazacyclononane-1,4-diacetic acid-c(RGDyK)-Glu-6-aminohexanoic acid-bombesin[7-14]NH_2_
Abbreviated name: | ^64^Cu-NO2A-RGD-Glu-6-Ahx-BBN
Synonym:
Agent category: | Peptide
Target: | Gastrin-releasing peptide receptor (GRPR), integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal\contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD)]

The amphibian bombesin (BBN or BN, a peptide of 14 amino acids) is an analog of human gastrin-releasing peptide (GRP, a peptide of 27 amino acids) that binds to GRP receptor (GRPR) with high affinity and specificity (1, 2). Both GRP and BBN share an amidated C-terminus sequence homology of seven amino acids, Trp-Ala-Val-Gly-His-Leu-Met-NH_2_. BBN-Like peptides have been shown to induce various biological responses in diverse tissues, including the central nervous system (CNS) and the gastrointestinal (GI) system. They also act as potential growth factors for both normal and neoplastic tissues (3). Specific BBN receptors (BBN-Rs) have been identified on CNS and GI tissues and on a number of tumor cell lines (4). The BBN-R superfamily includes at least four different subtypes, namely the GRPR subtype (BB2), the neuromedin B receptor subtype (BB1), the BB3 subtype, and the BB4 subtype. The findings of GRPR overexpression in various human tumors, such as breast, prostate, lung, colon, ovarian, and pancreatic cancers, provide opportunities for tumor imaging by designing specific molecular imaging agents to target the GRPR (5, 6).

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (7). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (8-13). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. A peptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various ligands have been introduced for imaging of tumors and tumor angiogenesis (14).

Because breast and prostate cancers express both GRPR and α_v_β_3_, Jackson et al. (15) designed an RGD-BBN heterodimer in which c(RGDyK) and BBN[7-14]NH_2_ are connected with a glutamate linker (BBN on the Glu side chain γ-carboxylate group and RGD on the Glu side chain α-carboxylate group). A spacer, 6-aminohexanoic acid (6-Ahx), was put onto the glutamate α-amino group of RGD-Glu-BBN to increase the hydrophilicity and to relieve the steric hindrance. 1,4,7-Triazacyclononane-1,4-7-triacetic acid (NOTA) was used as a bifunctional chelator for labeling RGD-BBN to form ^64^Cu-NO2A-RGD-Glu-6-Ahx-BBN for use in positron emission tomography (PET) imaging of α_v_β_3_ and GRPR in nude mice bearing human tumors.

### Related Resource Links:

- Chapters in MICAD (GRPR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=(GRPR%20OR%20GRP-R)%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (GRPR (http://www.ncbi.nlm.nih.gov/gene/2925), GRP (http://www.ncbi.nlm.nih.gov/gene/2922), α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (GRPR (http://www.ncbi.nlm.nih.gov/omim/305670), GRP (http://omim.org/entry/137260), α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (GRPR (http://www.clinicaltrials.gov/ct2/results?term=bombesin), RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+synthesis)]

RGD-Glu-6-Ahx-BBN was prepared with solid-phase peptide synthesis with the subsequent addition of a NOTA group to form NO2A-RGD-Glu-6-Ahx-BBN (15). Addition of a NOTA group to RGD-BBN was performed by mixing 2.7 µmol RGD-Glu-6-Ahx-BBN with an active ester. NO2A-RGD-Glu-6-Ahx-BBN was purified with high-performance liquid chromatography (HPLC), with ~70% yield. ^64^Cu-NO2A-RGD-Glu-6-Ahx-BBN was prepared by incubation of ^64^CuCl_2_ and NO2A-RGD-Glu-6-Ahx-BBN (24.2 nmol) in ammonium acetate buffer (pH 7) for 60 min at 70°C. ^64^Cu-NO2A-RGD-Glu-6-Ahx-BBN was purified with HPLC, with a radiochemical purity of >95%. The radiochemical yield, specific activity, and total preparation time were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+in+vitro)]

Jackson et al. (15) performed in vitro inhibition studies of NO2A-RGD-Glu-6-Ahx-BBN and ^nat^Cu-NO2A-RGD-Glu-6-Ahx-BBN in cultured human prostate cancer PC-3 cells with ^123^I-[Tyr^4^]-BBN, with 50% inhibition concentration (IC_50_) values of 3.99 ± 0.35 and 8.98 ± 1.34 nM, respectively. On the other hand, ^nat^Cu-NO2A-RGD showed minimal displacement of ^125^I-echistatin in PC-3 cells, suggesting that the cell binding of ^nat^Cu-NO2A-RGD-Glu-6-Ahx-BBN in PC-3 cells was primarily mediated by GRPR. In vitro internalization of ^64^Cu-NO2A-RGD-Glu-6-Ahx-BBN in PC-3 cells was performed at 37°C for 120 min. There was a gradual increase in the amount of radioactivity inside the cells, with ~1% of incubation dose at 120 min. Incubation with excess NO2A-RGD-6-Ahx-BBN and NO2A-RGD reduced cellular accumulation by 61% and 65%, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=BBN+RGD+%20rodentia)]

Jackson et al. (15) performed ex vivo biodistribution studies in nude mice (n = 4/group) bearing PC-3 xenografts at 1, 4, and 24 h after injection of 0.75 MBq (0.02 mCi) ^64^Cu-NO2A-RGD-Glu-6-Ahx-BBN. The organ with the highest accumulation was the pancreas, followed by the liver, kidney, intestine, stomach, blood, and muscle. The initial accumulation in the PC-3 tumors was 3.96 ± 1.36% injected dose/gram (ID/g) at 1 h, 2.18 ± 0.31% ID/g at 4 h, and 2.42 ± 0.57% ID/g at 24 h after injection. The organ with the highest radioactivity was the pancreas (21.65% ID/g at 1 h), followed by the large intestine (6.86% ID/g at 4 h), small intestine (5.21% ID/g at 1 h), kidney (4.65% ID/g at 1 h), urinary bladder (3.39% ID/g at 1 h), stomach (1.43% ID/g at 1 h), and liver (1.04% ID/g at 1 h). Most organs showed rapid clearance by 4 h or 24 h. The blood levels of radioactivity were 0.72%, 0.16%, and 0.18% ID/g at 1, 4, and 24 h, respectively. The tumor/blood ratios were 9.2, 21.8, and 22.0 at 1, 4, and 24 h, respectively. No blocking studies were performed.

PET scans were performed after intravenous injection of 26 MBq (700 μCi) ^64^Cu-NOTA-RGD-Glu-6-Ahx-BBN in one nude mouse bearing PC-3 tumor at 15 h after injection (15). PET/CT images showed that the radioactivity distribution pattern was consistent with the ex vivo biodistribution data. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=RGD+BBN+human)]

No publication is currently available.

## References

1 Gonzalez N., Moody T.W., Igarashi H., Ito T., Jensen R.T. (2008). Bombesin-related peptides and their receptors: recent advances in their role in physiology and disease states. Curr Opin Endocrinol Diabetes Obes.
2 Bertaccini G. (1976). Active polypeptides of nonmammalian origin. Pharmacol Rev.
3 Chung D.H., Evers B.M., Beauchamp R.D., Upp J.R., Rajaraman S., Townsend C.M., Thompson J.C. (1992). Bombesin stimulates growth of human gastrinoma. Surgery.
4 Benya R.V., Kusui T., Pradhan T.K., Battey J.F., Jensen R.T. (1995). Expression and characterization of cloned human bombesin receptors. Mol Pharmacol.
5 Reubi J.C., Wenger S., Schmuckli-Maurer J., Schaer J.C., Gugger M. (2002). Bombesin receptor subtypes in human cancers: detection with the universal radioligand (125)I-[D-TYR(6), beta-ALA(11), PHE(13), NLE(14)] bombesin(6-14). Clin Cancer Res.
6 Weiner R.E., Thakur M.L. (2005). Radiolabeled peptides in oncology: role in diagnosis and treatment. BioDrugs.
7 Hynes R.O. (2002). A reevaluation of integrins as regulators of angiogenesis. Nat Med.
8 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
9 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
10 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
11 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
12 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
13 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
14 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
15 Jackson A.B., Nanda P.K., Rold T.L., Sieckman G.L., Szczodroski A.F., Hoffman T.J., Chen X., Smith C.J. (2012). 64Cu-NO2A-RGD-Glu-6-Ahx-BBN(7-14)NH2: a heterodimeric targeting vector for positron emission tomography imaging of prostate cancer. Nucl Med Biol.